# 4-[^18^F]Fluorobenzoyl-NAVPNLRGDLQVLAQKVART

Chemical name: | 4-[^18^F]Fluorobenzoyl-NAVPNLRGDLQVLAQKVART
Abbreviated name: | [^18^F]FB-A20FMDV2
Synonym:
Agent Category: | Peptide
Target: | Integrin α_v_β_6_
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=A20FMDV2)]

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (1). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). Expression of the α_v_β_3_ integrin is strong on tumor cells and activated endothelial cells, whereas expression is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (6, 8, 9). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) has been identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins, including α_v_β_3_ and α_v_β_6_. Various radiolabeled antagonists have been introduced for imaging of tumors and tumor angiogenesis (10).

The α_v_β_6_ integrin plays an important role in the development of epithelial cells and is nearly undetectable in adult normal tissues. However, levels of the α_v_β_6_ integrin can be upregulated during tissue remodeling and wound healing (11). On the other hand, α_v_β_6_ integrin is strongly expressed on tumor cells of the oral cavity, pancreas, breast, ovary, colon, and stomach (12-14). The α_v_β_6_ integrin affects tumor growth, tumor invasiveness, and metastasis (13). α_v_β_6_ binds to the RGD motif in fibronectin, tenascin, and the viral protein 1 (VP1) of the foot-and-mouth disease virus (FMDV) (15). FMDV binds to cells through the RGD motif of the GH loop of the VP1. A consensus α_v_β_6_-binding motif DLXXL was identified with phage display screening with minimal binding to α_v_β_3_, α_IIb_β_3_, and α_v_β_5_ (16). A peptide of 20 amino acids, NAVPNLRGDLQVLAQKVART (A20FMDV2), was identified as a ligand binding to α_v_β_6_ integrin (15). A20FMDV2 was radiolabeled with N-succinimidyl 4-[^18^F]fluorobenzoate ([^18^F]SFB) to study in vivo biodistribution of the tracer in tumor-bearing mice (17). [^18^F]FB-A20FMDV2 was found to have specific accumulation in α_v_β_6_-positive tumor.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20A20FMDV2%20and%20synthesis)]

Hausner et al. (17) reported that of [^18^F]FB-A20FMDV2. A20FMDV2 was prepared by standard solid-phase peptide synthesis. [^18^F]SFB was synthesized in two steps from ethyl 4-(trimethylammoniumtrifluoromethanesulfonate) benzoate by nucleophilic fluorination ([^18^F]KF/Kryptofix 2.2.2./K_2_CO_3_), followed by saponification of the ethyl ester protecting group in 50 min using a chemistry process control unit with >99% radiochemical purity. The decay-corrected yields of [^18^F]SFB were 70% on the basis of starting [^18^F]KF. [^18^F]SFB was used to conjugate the N-terminus of A20FMDV2 in solid phase to form [^18^F]FB-A20FMDV2. Radiochemical purities of >98% were obtained with a decay-corrected radiochemical yield of 3.6% after high-performance liquid chromatography purification. The specific activity of [^18^F]FB-A20FMDV2 (n = 13) was 37 GBq/μmol (1 Ci/μmol) at end of synthesis with a total synthesis time of 130 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20A20FMDV2%20and%20%28in%20vitro%20or%20cell%29)]

Using competitive binding to immobilized α_v_β_6_, A20FMDV2 and FB-A20FMDV2 exhibited similar 50% inhibition concentration values (3 ± 1 nM) to inhibit α_v_β_6_-fibronetin binding, >1,000-fold more selective for α_v_β_6_ than for other RGD-directed integrins (α_5_β_1_, α_v_β_3_, and α_v_β_5_) (17). A receptor-binding assay with biotinylated A20FMDV2 using human melanoma DX3puro (α_v_β_6_-negative) and DX3puroβ_6_ (α_v_β_6_-positive) cell lines was analyzed with flow cytometry. The α_5_β_1_, α_v_β_3_, α_v_β_5_, α_v_β_6_, and α_v_β_8_ integrins were present on both cell lines. A20FMDV2 bound well at 1–100 nM to DX3puroβ_6_ cells but not to DX3puro, which suggests that A20FMDV2 is highly selective for α_v_β_6_.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20A20FMDV2%20and%20rodentia)]

Hausner et al. (17) performed biodistribution studies of [^18^F]FB-A20FMDV2 in nude mice (n = 3/group) bearing DX3puroβ_6_ and DX3puro xenografts on opposite flanks in the shoulder region. Data were obtained at 1, 2, and 4 h after injection. [^18^F]FB-A20FMDV2 had a rapid blood clearance with 0.27, 0.06, and 0.03% injected dose (ID)/g at 1, 2, and 4 h. The tracer radioactivity accumulation in the α_v_β_6_-expressing DX3puroβ_6_ tumor was ~0.66% ID/g at 1 h and decreased to 0.28% ID/g at 2 h and 0.06% ID/g at 4 h. The tracer radioactivity accumulation in the α_v_β_6_-negative DX3puro tumor was ~0.21% ID/g at 1 h and decreased to 0.07% ID/g at 2 h and 0.02% ID/g at 4 h. At 60 min, the highest radioactive concentration was found in the urine (1,082% ID/g), followed by the gallbladder (15% ID/g) and kidneys (3.6% ID/g). The spleen, bone, and liver showed low levels of radioactivity. [^18^F]FB-A20FMDV2 positron emission tomography imaging studies were performed at 15 min to 5 h after injection in mice (n = 6) bearing both tumors. The DX3puroβ_6_ tumor was clearly visualized as early as 15 min and as late as 5 h after injection. Considerable radioactivity accumulation was observed in the urinary bladder (urine), gallbladder, and kidneys. Tumor/background ratios were ~1.0 (DX3puro) and 2.2 (DX3puroβ_6_) at 1 h after injection. Pre-administration of unlabeled FB-A20FMDV2 blocked tumor uptake of radioactivity by 32% in the DX3puroβ_6_ tumor and <1% in the DX3puro tumor. The partial inhibition exhibited by the DX3puroβ_6_ tumor may be caused by the rapid blood and renal clearance of FB-A20FMDV2. Both tumors showed a similar accumulation of the metabolic tracer 2-[^18^F]fluoro-2-deoxy-D-glucose ([^18^F]FDG).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20A20FMDV2%20and%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20A20FMDV2%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=18F%20A20FMDV2%20and%20%28human%20not%20cell%29)]

No publication is currently available.

## References

1 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
2 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
3 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
4 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
5 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
6 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
7 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
11 Breuss J.M., Gallo J., DeLisser H.M., Klimanskaya I.V., Folkesson H.G., Pittet J.F., Nishimura S.L., Aldape K., Landers D.V., Carpenter W., et al. (1995). Expression of the beta 6 integrin subunit in development, neoplasia and tissue repair suggests a role in epithelial remodeling. J Cell Sci.
12 Thomas G.J., Nystrom M.L., Marshall J.F. (2006). Alphavbeta6 integrin in wound healing and cancer of the oral cavity. J Oral Pathol Med.
13 Kawashima A., Tsugawa S., Boku A., Kobayashi M., Minamoto T., Nakanishi I., Oda Y. (2003). Expression of alphav integrin family in gastric carcinomas: increased alphavbeta6 is associated with lymph node metastasis. Pathol Res Pract.
14 Bates R.C. (2005). The alphaVbeta6 integrin as a novel molecular target for colorectal cancer. Future Oncol.
15 DiCara D., Rapisarda C., Sutcliffe J.L., Violette S.M., Weinreb P.H., Hart I.R., Howard M.J., Marshall J.F. (2007). Structure-function analysis of Arg-Gly-Asp helix motifs in alpha v beta 6 integrin ligands. J Biol Chem.
16 Kraft S., Diefenbach B., Mehta R., Jonczyk A., Luckenbach G.A., Goodman S.L. (1999). Definition of an unexpected ligand recognition motif for alphav beta6 integrin. J Biol Chem.
17 Hausner S.H., DiCara D., Marik J., Marshall J.F., Sutcliffe J.L. (2007). Use of a peptide derived from foot-and-mouth disease virus for the noninvasive imaging of human cancer: generation and evaluation of 4-[18F]fluorobenzoyl A20FMDV2 for in vivo imaging of integrin alphavbeta6 expression with positron emission tomography. Cancer Res.